# Mesenchymal-epithelial transition factor binding peptide-8-aminooctanoic acid conjugated to Cy5.5

Chemical name: | Mesenchymal-epithelial transition factor binding peptide-8-aminooctanoic acid conjugated to Cy5.5 | Lys-Ser-Leu-Ser-Arg-His-Asp-His-Ile-His-His-His-aminooctanoic acid-Cys
Abbreviated name: | c-MBP-AOC-Cy5.5 | Lys-Ser-Leu-Ser-Arg-His-Asp-His-Ile-His-His-His-aminooctanoic acid-Cys
Synonym: | | Lys-Ser-Leu-Ser-Arg-His-Asp-His-Ile-His-His-His-aminooctanoic acid-Cys
Agent Category: | Ligand | Lys-Ser-Leu-Ser-Arg-His-Asp-His-Ile-His-His-His-aminooctanoic acid-Cys
Target: | Mesenchymal-epithelial transition factor receptor (c-Met); hepatocyte growth factor receptor (HGFR) | Lys-Ser-Leu-Ser-Arg-His-Asp-His-Ile-His-His-His-aminooctanoic acid-Cys
Target Category: | Receptor | Lys-Ser-Leu-Ser-Arg-His-Asp-His-Ile-His-His-His-aminooctanoic acid-Cys
Method of detection: | Near-infrared fluorescence (NIR) imaging | Lys-Ser-Leu-Ser-Arg-His-Asp-His-Ile-His-His-His-aminooctanoic acid-Cys
Source of signal / contrast: | Cy5.5 | Lys-Ser-Leu-Ser-Arg-His-Asp-His-Ile-His-His-His-aminooctanoic acid-Cys
Activation: | No | Lys-Ser-Leu-Ser-Arg-His-Asp-His-Ile-His-His-His-aminooctanoic acid-Cys
Studies: | - In vitro; - Rodents | Structure of cMBP-AOC-Cy5.5.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cMBP-GGG-Cy5.5)]

The hepatocyte growth factor (HGF) is the only known ligand of the mesenchymal-epithelial transition factor (c-Met) (also known as the HGF receptor) that has an important function, including cell development, proliferation, scattering, migration, and angiogenesis, all of which are necessary for the survival and repair of tissues (1). c-Met is known to mediate its activity through an intracellular tyrosine kinase (TK) that activates different signal transduction pathways, leading to initiation of the various cell processes (2). Also, deregulation of c-Met activity due to paracrine/autocrine activation, overexpression, or a mutation promotes the development of a neoplastic cell phenotype (2). Overexpression of c-Met and HGF has been associated with a poor prognosis and survival of the patient (3), suggesting that the c-Met receptor may be a suitable target for the detection of cancers at an early stage, which could help in the development of an appropriate treatment regimen to improve patient prognosis (4). c-Met is the target of several drugs under evaluation in clinical trials (http://clinicaltrials.gov/ct2/results?term=HGFR) approved by the United States Food and Drug Administration. Investigators recently generated a monoclonal antibody (mAb) that inhibits the HGF–c-Met interaction and identified the active mAb epitope peptide as KSLSRHDHIHHH, which was designated as the c-Met binding peptide (cMBP) (5). The cMBP and its derivatives (containing either a tri-amino acid linker, Gly-Gly-Gly (GGG), or an aliphatic carbon linker, 8-aminooctanoic acid (AOC)) were labeled with ^125^I to generate ^125^I-cMBP, 1^25^I-cMBP-GGG, and ^125^I-cMBP-AOC, and these agents were used to detect c-Met TK-positive tumor xenografts in mice (6). From this study the investigators concluded that although ^125^I-cMBP-AOC was a suitable imaging agent , and superior to 1^25^I-cMBP-GGG for the imaging of c-Met–expressing tumors, the imaging signal to background ratio could probably be improved further either by changing the linker in the molecule or by using a different nuclide or source of signal (such as an optical imaging agentIn an attempt to generate a c-Met–positive tumor imaging agent superior to ^125^I-cMBP-AOC, investigators conjugated a near-infrared (NIR) fluorescent dye, cyanine 5.5 (Cy5.5), to cMBP-GGG and cMBP-AOC to obtain cMBP-GGG-Cy5.5 and cMBP-AOC-Cy5.5 (4). The Cy5.5-conjugated cMBP derivatives were then evaluated for the NIR imaging of c-Met–positive xenograft tumors in a mouse model.

This chapter describes the characterization of only cMBP-AOC-Cy5.5. The other c-Met imaging agents (^125^I-cMBP, 1^25^I-cMBP-GGG, ^125^I-cMBP-AOC, and cMBP-GGG-Cy5.5) are described in separate MICAD chapters (7-10).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20synthesis)]

The synthesis of cMBP and cMBP-AOC-Cy5.5 has been described previously (4). Briefly, the cMBP-AOC peptide was synthesized using Fmoc chemistry, and it was mixed with Cy5.5-maleimide for 6 h in the dark at room temperature. The AOC linker was bound to the C-terminus of cMBP and Cy5.5 was linked to the C-terminus of AOC. The crude cMBP-AOC-Cy5.5 product was purified with dialysis using a 2,000 molecular weight cut-off membrane. The typical yield of cMBP-AOC-Cy5.5 was reported to be >65%. The molecular mass of the purified cMBP-AOC-Cy5.5 was determined with matrix-assisted laser desorption/ionization time-of-flight mass spectroscopy. The final product was analyzed with reverse-phase high-performance liquid chromatography (RP-HPLC). The purity of cMBP-AOC-Cy5.5 was reported to be >90% as determined with RP-HPLC. The absorption and fluorescence characteristics of cMBP-AOC-Cy5.5 were determined in water with the use of an ultraviolet-visible spectrophotometer, and the agent’s spectra were reported to be similar to that of free Cy5.5. Stability of the Cy5.5-labeled peptide was not reported.

For some in vitro studies, ^125^I-labeled cMBP was also used, and this radiolabeled compound was prepared as described before (6).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed]

A soluble human c-Met/Fc chimeric protein was purchased from a commercial source and used for an in vitro ^125^I-cMBP displacement binding assay using cMBP and cMBP-AOC-Cy5.5, respectively (4). The 50% inhibitory concentration values of cMBP and cMBP-AOC-Cy5.5 were determined to be 1.5 μM and 342 nM, respectively.

In another study, human U87MG glioma cells were exposed to cMBP-AOC-Cy5.5 (2 nmol) in the presence of excess unlabeled cMBP (86 nmol) and fluorescence was acquired 1 h later (4).Cells exposed to cMBP-AOC-Cy5.5 alone were reported to show fluorescence that was inhibited by the presence of excess unlabeled cMBP. Confocal microscopy revealed that cMBP-AOC-Cy5.5 bound only to the cell surface and was not internalized by the cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cMBP-GGG-Cy5.5+rodentia)]

NIR fluorescence imaging was performed on athymic mice (the number of animals used per time point was not reported) bearing U87MG cell xenograft tumors at predetermined time points for up to 24 h after injection of cMBP-AOC-Cy5.5 through the tail vein (4). For comparison, another group of animals was injected with cMBP-GGG-Cy5.5. Fluorescence imaging of the two groups of animals showed that the signals from both conjugates were visible primarily in the tumor, kidney, and the bladder regions of the animals. The tumor/muscle (T/M) ratios for the two conjugates were generated for the different time points after imaging. With cMBP-AOC-Cy5.5, the ratio was observed to increase from ~3 at 10 min to ~33 at 17 h, and it remained stable thereafter for up to 24 h. A similar trend was noticed with cMBP-GGG-Cy5.5, but the fluorescence with this conjugate was consistently approximately three-fold lower than that obtained with cMBP-AOC-Cy5.5, indicating that the latter was a superior imaging agent for c-Met-expressing tumors compared with cMBP-GGG-Cy5.5. Blocking studies were performed by co-injecting the mice with cMBP-AOC-Cy5.5 in the absence or presence of excess cMBP (0.13 μmol) followed by imaging at designated time points as before. Compared with animals injected with cMBP-AOC-Cy5.5 alone, a low fluorescence signal was obtained (at all time points) from animals injected with the peptide mixture. This indicated that cMBP blocked the binding of cMBP-AOC-Cy5.5 to the xenograft tumors. To study the biodistribution of cMBP-AOC-Cy5.5 in the xenograft tumor mice, animals from the blocking study were euthanized after imaging, and all the major organs were collected to determine the amount of fluorescent dye accumulated in the tissues (4). Compared with all the harvested organs, a high signal was obtained from the tumor and kidneys of the animals, but the signal was reduced only in tumors from the blocked animals. From these studies the investigators concluded that cMBP-AOC-Cy5.5 was a superior imaging agent for c-Met-expressing tumors compared with cMBP-GGG-Cy5.5.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cMBP-GGG-Cy5.5+Non-Primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cMBP-GGG-Cy5.5+Non-Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cMBP-GGG-Cy5.5+Human+Studies)]

No references are currently available.

## Supplemental Information

[Disclaimer]

No information is currently available.

## References

1 Naran S., Zhang X., Hughes S.J. (2009). Inhibition of HGF/MET as therapy for malignancy. Expert Opin Ther Targets.
2 Abounader R., Laterra J. (2005). Scatter factor/hepatocyte growth factor in brain tumor growth and angiogenesis. Neuro Oncol.
3 Birchmeier C., Birchmeier W., Gherardi E., Vande Woude G.F. (2003). Met, metastasis, motility and more. Nat Rev Mol Cell Biol.
4 Kim E.M., Park E.H., Cheong S.J., Lee C.M., Jeong H.J., Kim D.W., Lim S.T., Sohn M.H. (2009). In vivo imaging of mesenchymal-epithelial transition factor (c-Met) expression using an optical imaging system. Bioconjug Chem.
5 Kim K., Hur Y., Ryu E.K., Rhim J.H., Choi C.Y., Baek C.M., Lee J.H., Chung J. (2007). A neutralizable epitope is induced on HGF upon its interaction with its receptor cMet. Biochem Biophys Res Commun.
6 Kim E.M., Park E.H., Cheong S.J., Lee C.M., Kim D.W., Jeong H.J., Lim S.T., Sohn M.H., Kim K., Chung J. (2009). Characterization, biodistribution and small-animal SPECT of I-125-labeled c-Met binding peptide in mice bearing c-Met receptor tyrosine kinase-positive tumor xenografts. Nucl Med Biol.
7 Chopra, A., 125I labeled mesenchymal-epithelial transition factor binding peptide [125I-cMBP]. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
8 Chopra, A., 125I labeled mesenchymal-epithelial transition factor binding peptide-Gly-Gly-Gly. [125I-cMBP-GGG]. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
9 Chopra, A., 125I labeled mesenchymal-epithelial transition factor binding peptide-8-aminooctanoic acid linker. [125I-cMBP-AOC]. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
10 Chopra, A., Mesenchymal-epithelial transition factor binding peptide-Gly-Gly-Gly-conjugated to Cy5.5 [cMBP-GGG-Cy5.5]. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.